# ^99m^Tc-Hydrazinonicotinic acid-bitistatin

Chemical name: | ^99m^Tc-Hydrazinonicotinic acid-bitistatin
Abbreviated name: | ^99m^Tc-HYNIC-bitistatin
Synonym:
Agent category: | Polypeptide
Target: | Platelet glycoprotein GPIIb/IIIa receptor (CD61/CD41)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Bitistatin)]

Thrombosis plays a major role in many cardiovascular diseases such as myocardial infarction, pulmonary embolism (PE), deep venous thrombosis (DVT), or cerebral venous thrombosis (1, 2). DVT is a significant source of PE, which is a potentially life-threatening clinical problem. Thrombosis occurs when platelets deposit in regions of low flow in the deep venous system, followed by an activation process of thrombin, which then converts fibrinogen into fibrin. Platelets become activated and bind to fibrinogen, resulting in platelet aggregation. The thrombus may become organized or detached from the vessel wall. Bitistatin (83 amino acids) belongs to a family of platelet glycoprotein GPIIb/IIIa ligands called disintegrins, which contain an Arg-Gly-Asp (RGD) tripeptide sequence (3). Bitistatin has been shown to inhibit platelet deposition in coronary arteries in a canine model of repetitive thrombus formation (4). ^99m^Tc-Hydrazinonicotinic acid-bitistatin (^99m^Tc-HYNIC-bitistatin) is being developed as a single-photon emission computed tomography (SPECT) imaging probe for imaging of acute thrombi and emboli in humans.

### Related Resource Links:

- Chapters in MICAD (GPIIb (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=GPIIb+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/gene/3690), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/gene/3674))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=173470), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=607759))
- Clinical trials (Integrin (http://www.clinicaltrials.gov/ct2/results?term=integrin))
- Drug information in FDA (Integrin (http://google2.fda.gov/search?q=integrin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=17&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Bitistatin+and+synthesis)]

Knight et al. (5) reported a two-step synthesis of ^99m^Tc-HYNIC-bitistatin using the bifunctional chelating agent N-succinimidyl-HYNIC, a ligand with two active sites: one for protein conjugation with the amino groups on lysine residues of bitistatin, and the other for coordination of ^99m^Tc. Bitistatin (0.22 mmol) was incubated for 90 min at room temperature with excess of N-succinimidyl-HYNIC (8.8 mmol). There were ~2 HYNIC molecules per bitistatin. After purification, 4.2 GBq/ml (113 mCi) of ^99m^Tc-glucoheptonate was mixed with HYNIC-bitistatin. The mixture was incubated at for 30 min room temperature. Radiochemical purity was >97% after high-performance liquid chromatography with a specific activity of 96 TBq/mmol (2,600 Ci/mmol). Recombinant bitistatin (rBitistatin) has recently been radiolabeled with ^99m^Tc-pertechnetate, using tricine as a coligand, with a radiochemical purity of >90% and a specific activity of up to 333 TBq/mmol (9,000 Ci/mmol) (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Bitistatin+and+in+vitro)]

In a saturation binding experiment, ^99m^Tc-HYNIC-bitistatin exhibited a binding constant (K_d_) of 32 ± 1 nM in human stimulated platelets, whereas resting platelets exhibited a K_d_ value of 62 ± 9 nM (5). On the other hand, there was no difference in the number of binding sites per platelet (B_max_) between stimulated and resting platelets. ^99m^Tc-HYNIC-bitistatin had similar binding affinity to that of ^125^I-bitistatin (41 ± 5 and 56 ± 5 nM for stimulated and resting platelets, respectively).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Bitistatin+and+rodentia)]

Knight et al. (6) performed biodistribution studies of ^99m^Tc-HYNIC-rBitistatin in normal mice. The highest radioactivity concentrations were observed in the kidneys (90.9% injected dose per gram (ID/g)), spleen (10.6% ID/g), lungs (8.0% ID/g), blood (7.2% ID/g), and liver (4.8% ID/g) at 15 min after injection. With the exception of the intestines, all other organs and tissues showed a continuing decrease in radioactivity with time up to 4 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Bitistatin+and+(dog+or+sheep+or+pig+or+rabbit))]

Knight et al. (6) performed biodistribution studies of ^99m^Tc-HYNIC-rBitistatin in normal dogs. The highest radioactivity concentrations were observed in the kidneys (40.3% ID/organ), blood (23.42% ID/organ), liver (12.5% ID/organ) lungs (6.49% ID/organ), and spleen (3.75% ID/organ) at 4 h after injection; 87% of blood radioactivity was bound to platelets. Urine excretion averaged 23% of ID by 4 h after injection.

Knight et al. (5) performed SPECT planar imaging in dogs (n = 6) with DVT and PE induced by placing thrombogenic embolization coils in the right femoral vein. In vivo, focal uptake was observed as early as 30 min (DVT) and 60 min (PE) after injection. Lesion uptake of ^99m^Tc-HYNIC-bitistatin at 4 h after injection averaged 0.89 ± 0.34% ID/g PE and 0.79 ± 0.23% ID/g DVT. Lesion/background ratios averaged 27 ± 13 (PE/blood), 34 ± 12 (PE/lung), 18 ± 4 (DVT/blood), and 284 ± 97 (DVT/muscle). The blood clearance pattern exhibited a two-phase model with a half-life (t_1/2_α) of 8.9 min during the distribution phase and a half-life (t_1/2_ß) of 5.8 h during the elimination phase.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Bitistatin+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Bitistatin+and+human)]

Knight et al. (6) performed ^99m^Tc-HYNIC-rBitistatin scintigraphy in 4 normal volunteers. The blood clearance pattern exhibited a two-phase model with a distribution half-life t_1/2_α of 6.6 min and an elimination half-life t_1/2_ß of 3.8 h. The organ with the highest accumulation was the kidney (5.3% ID), followed by the liver (4.1% ID) and spleen (2.7% ID) at 1 h. Urine excretion averaged 30% of ID by 4 h after injection. The effective dose equivalent was estimated to be 5.4 μSv/MBq (19.9 mrem/mCi) for adult males and 7.1 μSv/MBq (26.2 mrem/mCi) for adult females.

## NIH Support

R01 HL54578, R01 HL054578-07, CA16520, DK19525

## References

1 Corti R., Fuster V. (2003). New understanding, diagnosis, and prognosis of atherothrombosis and the role of imaging. Am J Cardiol.
2 Taillefer R. (2001). Radiolabeled peptides in the detection of deep venous thrombosis. Semin Nucl Med.
3 Knight L.C., Romano J.E. (2005). Functional expression of bitistatin, a disintegrin with potential use in molecular imaging of thromboembolic disease. Protein Expr Purif.
4 Shebuski R.J., Ramjit D.R., Bencen G.H., Polokoff M.A. (1989). Characterization and platelet inhibitory activity of bitistatin, a potent arginine-glycine-aspartic acid-containing peptide from the venom of the viper Bitis arietans. J Biol Chem.
5 Knight L.C., Baidoo K.E., Romano J.E., Gabriel J.L., Maurer A.H. (2000). Imaging pulmonary emboli and deep venous thrombi with 99mTc-bitistatin, a platelet-binding polypeptide from viper venom. J Nucl Med.
6 Knight L.C., Romano J.E., Cosenza S.C., Iqbal N.M., Marcinkiewicz C. (2007). Differences in binding of (99m)Tc-disintegrins to integrin alphavbeta3 on tumor and vascular cells. Nucl Med Biol.